# ^89^Zr-Desferrioxamine B-7E11 anti-prostate-specific membrane antigen monoclonal antibody

Chemical name: | ^89^Zr-Desferrioxamine B-7E11 anti-prostate-specific membrane antigen monoclonal antibody
Abbreviated name: | ^89^Zr-DFO-7E11
Synonym:
Agent category: | Antibody
Target: | Prostate-specific membrane antigen (PSMA), or N-acetyl α-linked acidic dipeptidase (NAALADase)
Target category: | Antigen
Method of detection: | Positron emission tomography (PET)
Source of signal: | ^89^Zr
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4758398), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=4758397) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2346) for more information about PSMA.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Zr%207E11)]

Prostate-specific membrane antigen (PSMA) is a cell-surface glycoprotein with a molecular weight of ~100 kDa. It is a unique, type II, transmembrane-bound glycoprotein that is overexpressed on prostate tumor cells and in the neovasculature of most solid prostate tumors, but not in the vasculature of normal tissues (1, 2). PSMA has also been detected in other tissues such as the kidneys, the proximal small intestine, and the salivary glands (2). PSMA has been found to have N-acetyl α-linked acidic dipeptidase (NAALADase) or glutamate carboxypeptidase II activity (3). PSMA may play an important role in the progression of prostate cancer and glutamatergic neurotransmission, as well as in the absorption of folate (4). In the central nervous system, PSMA metabolizes N-acetyl-aspartyl-glutamate, and in the proximal small intestine it removes γ-linked glutamates from poly-γ-glutamate folate and folate hydrolase (2). This unique expression of PSMA makes it an important biomarker as well as a large extracellular target of imaging agents (5, 6). PSMA can be used as a biomarker for the detection of prostate cancer with imaging agents.

7E11, a monoclonal antibody against the cytoplasmic domain of PSMA, has been found to be specific to prostate tumor tissues in humans (7). Tumors often contain dying or necrotic cells with permeable membranes, allowing the binding of antibodies to the intracellular epitope of PSMA. The antibody conjugate (capromab pendetide or CYT-365) was radiolabeled with ^111^In. ^111^In-Capromomab pendetide (http://www.ncbi.nlm.nih.gov/bookshelf/br.fcgi?book=micad&part=Capromab111In) was approved by the United States Food and Drug Administration in 1996 for the detection of prostate carcinoma and soft tissue metastases in prostate cancer patients (8). However, the results obtained with this antibody are not entirely reliable (9). In addition, this antibody has limited access to tumors and may produce low signal/noise ratios because the target is the intracellular domain of PSMA (10). Newer monoclonal antibodies (e.g., J591) against the extracellular domain of PSMA are being developed for imaging and immunotherapy of prostate cancer (11, 12). Ruggiero et al. (13) conjugated 7E11 with desferrioxamine B (DFO) and radiolabeled the product with ^89^Zr to form ^89^Zr-DFO-7E11 for positron emission tomography (PET) imaging of PSMA expression as a marker for dead or dying prostate tumor cells.

### Related Resource Links:

- Chapters in MICAD (PSMA (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=PSMA+AND+micad%5Bbook%5D))
- Gene information in NCBI (PSMA (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=2346))
- Articles in Online Mendelian Inheritance in Man (OMIM) (PSMA (http://www.ncbi.nlm.nih.gov/omim/602640))
- Clinical trials (PSMA (http://www.clinicaltrials.gov/ct2/results?term=PSMA), 7E11 (http://www.clinicaltrials.gov/ct2/results?term=7e11))
- Drug information in FDA (Capromab pendetide (http://google2.fda.gov/search?q=Capromab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=9&y=7))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Zr%207E11%20AND%20synthesis)]

7E11-C5 was coupled with N-SucDf via an amide linkage (13). DFO-7E11 was purified with column chromatography. DFO-7E11 (4.9 nmol) was labeled with 138.8 MBq (3.75 mCi) ^89^Zr-oxalate for ~60 min at room temperature with a high yield of 89% (n = 4). ^89^Zr-DFO-7E11 was purified with spin-column centrifugation and retained 89% immunoreactivity. The radiochemical purity was >95% with a specific activity was ~25 MBq/nmol (0.68 mCi/nmol). The number of DFO moieties per antibody was 2.6 ± 0.5. ^89^Zr-DFO-7E11 showed <2% loss of ^89^Zr and no loss of immunoreactivity in saline at 37°C for 7 d.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Zr%207E11%20AND%20in%20vitro)]

LNCaP human prostate cancer cells were reported to have a K_d_ value of 6.69 nM with [^131^I]7E11-C5 and a B_max_ value of 95,000 sites/cell in saturation binding studies (14) using intact cells. The binding was accounted for by a subpopulation of permeated cells produced when the cells were trypsinized and washed. Little internalization of the tracer was found over a period of 48 h at 37°C. When permeated cells were used, the number of binding sites/cell was similar to [^131^I]J591, an antibody against the extracellular domain of PSMA. Using nonpermeated cells, [^131^I]J591 has a K_d_ of 1.83 nM and a B_max_ of 600,000–800,000 sites/cell.

Ruggiero et al. (13) performed flow cytometry and fluorescence microscopy analysis of PSMA-positive prostate cancer cells after treatments with etoposide (chemotherapy), flutamide (anti-androgen hormonal therapy), and irradiation radiotherapy. There was an increase in the percentage of cells stained with 7E11 and 7-amino-actinomycin-D (7-AAD for cell membrane permeabilization and viability assessment) with all treatments over time (24–120 h). There was a colocalization of 7E11 and caspase 3 staining in the cells at 96 h after treatments.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Zr%207E11%20and%20rodentia)]

Ruggiero et al. (13) performed ex vivo biodistribution studies with 0.55–0.74 MBq (0.015–0.02 mCi, 20–26 pmol) ^89^Zr-DFO-7E11 in nude mice (n = 5 per group) bearing LnCaP (PSMA-positive) bilateral tumors. One of the tumors in each mouse received radiotherapy (20 Gy). The accumulation in the untreated LnCaP tumors was 20.4 ± 7.5% injected dose per gram (ID/g), 22.8 ± 3.6% ID/g, 37.0 ± 6.3% ID/g, and 25.2 ± 4.8% ID/g at 24, 48, 96, and 120 h after injection, respectively. The accumulation in the treated LnCaP tumors was 24.7 ± 7.2% ID/g, 40.6 ± 7.5% ID/g, 51.8 ± 7.4% ID/g, and 52.7 ± 11.1% ID/g at 24, 48, 96, and 120 h after injection, respectively. The higher accumulation values in the treated tumors than in the untreated tumors were statistically significant (P < 0.05) with the exception of the 24-h time point. The tissue with the highest accumulation at 48 h after injection was the liver (42.7% ID/g), followed by the spleen (29.9% ID/g), kidney (21.6% ID/g), lung (7.6% ID/g), bone (6.3% ID/g), intestine (4.9% ID/g), heart (4.7% ID/g), and muscle (1.0% ID/g). The radioactivity level in the blood was 32.6% ID/g at 24 h and declined to 6.6% ID/g at 120 h. The tumor/blood ratios were 1.8 and 1.0 at 48 h for the treated and untreated tumors, respectively. Coinjection with excess 7E11 (2.0 nmol) reduced the tumor/blood ratios by ~60% to 0.5 and 0.4 at 48 h for the treated and untreated tumors. Autoradiography studies of the tumor sections showed higher accumulation of ^89^Zr-DFO-7E11 in the treated tumors than in the untreated tumors. Immunochemical staining showed colocalization of 7E11 with apoptotic (caspase 3) and necrotic areas (hematoxylin and eosin) in the treated tumor sections.

PET imaging in nude mice (n = 5) with ~11 MBq (0.3 mCi) ^89^Zr-DFO-7E11 (0.44 nmol per mouse) visualized both the untreated and treated LnCaP tumors as early as 24 h after injection with a maximum contrast at 72 h (13). The accumulation in the untreated LnCaP tumors was 14.7 ± 5.7% ID/g, 14.7 ± 6.3% ID/g, 19.1 ± 7.3% ID/g, 15.6 ± 7.9% ID/g, and 14.8 ± 8.1% ID/g at 24, 48, 72, 96, and 120 h after injection, respectively. The accumulation in the treated LnCaP tumors was 21.6 ± 2.5% ID/g, 29.9 ± 2.3% ID/g, 31.8 ± 3.8% ID/g, 30.7 ± 5.0% ID/g, and 31.4 ± 5.3% ID/g at 24, 48, 72, 96, and 120 h after injection, respectively. The accumulation values in the treated tumors were significantly higher (P < 0.05) than in the untreated tumors at all the time points studied.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Zr%207E11%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Zr%207E11%20AND%20Primates)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Zr%207E11%20AND%20human)]

No publication is currently available.

## NIH Support

U24 CA83084, P30 CA008748-44S5, P30 CA08748, R25T CA096945

## References

1 Feneley M.R., Brewster S. (2003). Opportunities and outcomes in early prostate cancer: a commentary on policy, patient perspectives, trials and strategies. BJU Int.
2 Ghosh A., Heston W.D. (2004). Tumor target prostate specific membrane antigen (PSMA) and its regulation in prostate cancer. J Cell Biochem.
3 Luthi-Carter R., Barczak A.K., Speno H., Coyle J.T. (1998). Molecular characterization of human brain N-acetylated alpha-linked acidic dipeptidase (NAALADase). J Pharmacol Exp Ther.
4 O'Keefe D.S., Bacich D.J., Heston W.D. (2004). Comparative analysis of prostate-specific membrane antigen (PSMA) versus a prostate-specific membrane antigen-like gene. Prostate.
5 Nanus, D.M., M.I. Milowsky, L. Kostakoglu, P.M. Smith-Jones, S. Vallabahajosula, S.J. Goldsmith, and N.H. Bander, Clinical use of monoclonal antibody HuJ591 therapy: targeting prostate specific membrane antigen. J Urol, 2003170(6 Pt 2): p. S84-8; discussion S88-9.
6 Nargund V., Al Hashmi D., Kumar P., Gordon S., Otitie U., Ellison D., Carroll M., Baithun S., Britton K.E. (2005). Imaging with radiolabelled monoclonal antibody (MUJ591) to prostate-specific membrane antigen in staging of clinically localized prostatic carcinoma: comparison with clinical, surgical and histological staging. BJU Int.
7 Horoszewicz J.S., Kawinski E., Murphy G.P. (1987). Monoclonal antibodies to a new antigenic marker in epithelial prostatic cells and serum of prostatic cancer patients. Anticancer Res.
8 Bander N.H. (2006). Technology insight: monoclonal antibody imaging of prostate cancer. Nat Clin Pract Urol.
9 Ponsky L.E., Cherullo E.E., Starkey R., Nelson D., Neumann D., Zippe C.D. (2002). Evaluation of preoperative ProstaScint scans in the prediction of nodal disease. Prostate Cancer Prostatic Dis.
10 Jain R.K. (1999). Transport of molecules, particles, and cells in solid tumors. Annu Rev Biomed Eng.
11 Bander N.H., Trabulsi E.J., Kostakoglu L., Yao D., Vallabhajosula S., Smith-Jones P., Joyce M.A., Milowsky M., Nanus D.M., Goldsmith S.J. (2003). Targeting metastatic prostate cancer with radiolabeled monoclonal antibody J591 to the extracellular domain of prostate specific membrane antigen. J Urol.
12 Smith-Jones P.M., Vallabhajosula S., Navarro V., Bastidas D., Goldsmith S.J., Bander N.H. (2003). Radiolabeled monoclonal antibodies specific to the extracellular domain of prostate-specific membrane antigen: preclinical studies in nude mice bearing LNCaP human prostate tumor. J Nucl Med.
13 Ruggiero A., Holland J.P., Hudolin T., Shenker L., Koulova A., Bander N.H., Lewis J.S., Grimm J. (2011). Targeting the internal epitope of prostate-specific membrane antigen with 89Zr-7E11 immuno-PET. J Nucl Med.
14 Smith-Jones P.M., Vallabahajosula S., Goldsmith S.J., Navarro V., Hunter C.J., Bastidas D., Bander N.H. (2000). In vitro characterization of radiolabeled monoclonal antibodies specific for the extracellular domain of prostate-specific membrane antigen. Cancer Res.